# ^99m^Tc-Labeled imine 6-(pyridine-2-methylimine)-4-[(3-bromophenyl)amino]quinazoline

Chemical name: | ^99m^Tc-Labeled imine 6-(pyridine-2-methylimine)-4-[(3-bromophenyl)amino]quinazoline
Abbreviated name: | [^99m^Tc]Complex 7
Synonym:
Agent Category: | Compound
Target: | Epidermal growth factor receptor tyrosine kinase (EGFR TK)
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); planar gamma imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR-TK+imaging)]

The epidermal growth factor (EGF) receptor (EGFR)–associated tyrosine kinase (TK) is one of the most widely investigated enzymes of this category (1). Under normal conditions, autophosphorylation of the EGFR-TK, as a result of ligand (e.g., the EGF) binding to the receptor, initiates cellular signal transduction pathways that culminate in cell growth, proliferation, motility, and even differentiation into an oncogenic phenotype (2). Because of its participation in the development and spread of several cancer types, the EGFR and the EGFR-TK have been targeted for the treatment of various cancers using a variety of drugs including EGFR antibodies (http://clinicaltrials.gov/ct2/results?term=EGFR+antibodies) (3) and small molecule inhibitors (http://clinicaltrials.gov/ct2/results?term=EGFR+tyrosine+kinase+inhibitors) directed toward the TK (4). In addition, several of these agents are under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR+inhibitors) approved by the United States Food and Drug Administration.

The EGFR-TK inhibitors competitively bind to the intracellular ATP binding site of the enzyme and prevent autophosphorylation of the receptor, which thereby inhibits triggering of the signal transduction pathways responsible for initiation of the various biological processes mediated by the EGFR (5). Several types of reversible and irreversible EGFR-TK inhibitors are available, but among these the 4-anilinoquinazoline derivatives have been most widely investigated because of their higher potency compared with the other compounds (6). The 4-anilinoquinazoline class of inhibitors has been labeled with nuclides such as fluorine-18, carbon-11, and iodine-124 for positron emission tomography (PET) molecular imaging of the EGFR in animals (7). However, these labeled compounds were determined to be suboptimal for the studies either due to non-specificity of binding or due to rapid degradation in the blood and liver. In an effort to develop an imaging agent superior to the PET compounds, a technetium (^99m^Tc)–labeled quinazoline ([^99m^Tc]-imine 6-(pyridine-2-methylimine)-4-[(3-bromophenyl)amino]quinazoline ([^99m^Tc]complex 7)) was developed, and Bourkoula et al. studied its biodistribution in healthy mice (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR-TK+inhibitor+synthesis)]

The synthesis and labeling of complex 7 with ^99m^Tc was described in detail by Bourkoula et al. (6). The radiochemical yield of the reaction was reported to be 85–90% as determined with high-performance liquid chromatography. The radiochemical purity and specific activity of the labeled compound were not reported. The stability of [^99m^Tc]complex 7 was reported to be >95% for 24 h at room temperature, but in the presence of excess amounts of histidine or cysteine (molar ratio 1:1000) the stability was ~90% under these conditions during this period (6). Histidine and cysteine were also used to investigate the stability of the radiotracer because these amino acids are known to have a high affinity for the ^99m^Tc binding core of the compound and can degrade the molecule (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

Only the intermediate derivatives leading to the synthesis of [^99m^Tc]complex 7 were characterized for activity under in vitro conditions using human A431 epidermoid vulval carcinoma cells (6). These intermediate quinazoline derivatives had 50% inhibitory concentrations (IC_50_) ranging from 3.5 ± 1.1 to 114 ± 23 nM for the A431 cell EGFR autophosphorylation. The IC_50_ value for A431 cell growth was reported to range from 4.8 ± 0.2 to 2.0 ± 0.98 μM for the intermediate compounds.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR-TK+inhibitor+biodistribution)]

The biodistribution of [^99m^Tc]complex 7 was investigated in healthy Swiss albino mice (6). The animals (n = 4 per time point) were administered [^99m^Tc]complex 7 through the tail vein and euthanized 1, 15, 60, and 180 min after injection. The major organs of the animals were excised, weighed, and counted, and the amount of radioactivity accumulated in each organ was calculated as percent injected dose/gram tissue (% ID/g). A rapid clearance of [^99m^Tc]complex 7 from the blood was reported between 1 and 15 min, followed by a gradual decrease in radioactivity up to 180 min (21.51 ± 3.05, 6.10 ± 0.63, and 2.01 ± 0.24% ID/g, respectively). Accumulation of radioactivity (19.80 ± 1.55% ID/g) in the liver was observed up to 15 min after administration of the radiotracer followed by a decrease (9.53 ± 1.65% ID/g) by 180 min after the injection. During the same period an accumulation of radioactivity was noted in the intestines from 4.54 ± 0.57% ID/g at 15 min to 16.79 ± 1.19% ID/g at 180 min. The amount of radioactivity accumulated in the kidneys remained constant (8.14 ± 0.62% ID/g at 15 min to 8.16 ± 0.90 at 180% ID/g at 180 min) for the entire duration of the study. Radioactivity was reported to increase in the urine from 1.57 ± 0.40% ID/g at 15 min to 4.60 ± 0.57% ID/g. This study indicated that radioactivity derived from [^99m^Tc]complex 7 was excreted primarily through the hepatobiliary and the urinary routes.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR-TK+inhibitor+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR-TK+inhibitor+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=EGFR-TK+inhibitor+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

## References

1 Kumar A., Petri E.T., Halmos B., Boggon T.J. (2008). Structure and clinical relevance of the epidermal growth factor receptor in human cancer. J Clin Oncol.
2 Gusterson B.A., Hunter K.D. (2009). Should we be surprised at the paucity of response to EGFR inhibitors?. Lancet Oncol.
3 Heinemann V., Stintzing S., Kirchner T., Boeck S., Jung A. (2009). Clinical relevance of EGFR- and KRAS-status in colorectal cancer patients treated with monoclonal antibodies directed against the EGFR. Cancer Treat Rev.
4 Ansari J., Palmer D.H., Rea D.W., Hussain S.A. (2009). Role of tyrosine kinase inhibitors in lung cancer. Anticancer Agents Med Chem.
5 Linardou H., Dahabreh I.J., Bafaloukos D., Kosmidis P., Murray S. (2009). Somatic EGFR mutations and efficacy of tyrosine kinase inhibitors in NSCLC. Nat Rev Clin Oncol.
6 Bourkoula, A., M. Paravatou-Petsotas, A. Papadopoulos, I. Santos, H.J. Pietzsch, E. Livaniou, M. Pelecanou, M. Papadopoulos, and I. Pirmettis, Synthesis and characterization of rhenium and technetium-99m tricarbonyl complexes bearing the 4-[3-bromophenyl]quinazoline moiety as a biomarker for EGFR-TK imaging. Eur J Med Chem, 2009
7 Cai W., Niu G., Chen X. (2008). Multimodality imaging of the HER-kinase axis in cancer. Eur J Nucl Med Mol Imaging.